# 5-3’-[^18^F]Fluoropropyl-3-[2-((S)-pyrrolidinyl)methoxy]pyridine

Chemical name: | 5-3’-[^18^F]Fluoropropyl-3-[2-((S)-pyrrolidinyl)methoxy]pyridine
Abbreviated name: | [^18^F]Nifrolidine
Synonym:
Agent category: | Compound
Target: | α4β2 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolidine)]

Neuronal nicotinic cholinergic receptors (nAChRs) are a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine always causes a rapid increase in cellular permeability to ions such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α (α2–α10) and four subtypes of structural β (β2–β5). nAChRs have been demonstrated to be involved in cognitive processes such as learning, memory, and control of movement in normal subjects. Dysfunction of nAChRs has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction.

2-[^18^F]Fluoro-A-85380 (2-[^18^F]FA (http://www.ncbi.nlm.nih.gov/books/NBK23401/) and 6-[^18^F]FA (http://www.ncbi.nlm.nih.gov/books/NBK23587/)) (nAChR agonists) have been evaluated as positron emission tomography (PET) agents for the non-invasive study of nAChR in humans (4, 5). However, prolonged imaging times (2–4 h) are required for reliable quantification because of the slow kinetics of nAChR binding. 5-(3'-fluoropropyl)-3-(2-(S)-pyrrolidinylmethoxy)pyridine (nifrolidine) is a putative and selective nAChR antagonist with nanomolar affinity. An antagonist may provide additional and complementary information about nAChR beyond that obtained by an agonist-based radiotracer such as 2-[^18^F]FA. For example, an antagonist will measure total receptor, whereas an agonist will measure the high-affinity receptor. 5-(3'-[^18^F]-Fluoropropyl)-3-(2-(S)-pyrrolidinylmethoxy)pyridine ([^18^F]nifrolidine) is being developed as a PET agent with faster kinetics than 2-[^18^F]FA and 6-[^18^F]FA for the non-invasive study of nAChR in the brain.

### Related Resource Links:

- Chapters in MICAD (nACHR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nAChR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (nAChR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=1137)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (nAChR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=Neuronal%5BAll+Fields%5D+AND+nicotinic%5BAll+Fields%5D+AND+acetylcholine%5BAll+Fields%5D+AND+receptor%5BAll+Fields%5D))
- Clinical trials (nAChR (http://www.clinicaltrials.gov/ct2/results?term=nAChR))
- Drug information in FDA (nAChR (http://google2.fda.gov/search?q=Neuronal+nicotinic+acetylcholine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolidine%20and%20synthesis)]

Chattopadhyay et al. (6) reported synthesis of [^18^F]nifrolidine by a two-step reaction, which consisted of standard ^18^F-nucleophilic fluorination of 5-(3'-[(4-methylphenyl)sulfonyloxy]propyl)-3-(1-BOC-2-(S)-pyrrolidinylmethoxy)pyridine and acidic deprotection of the product. An average radiochemical yield was 20–40% (decay-corrected), with a total synthesis time of 150 min. Specific activities were 111–185 GBq/μmol (3–5 Ci/μmol) at the end of synthesis, with a radiochemical purity of >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolidine%20and%20in%20vitro)]

Pichika et al. (7) reported that nifrolidine, nifene, and nicotine had K_i_ values of 0.80 ± 0.11, 0.50 ± 0.14, and 1.68 ± 0.28 nM, respectively, in [^3^H]cytisine (α4β2 nicotinic acetylcholine receptor) binding assays using rat brain membranes. Using in vitro autoradiography studies of rat brain slices, Chattopadhyay et al. (6) reported that nifrolidine had a K_i_ value of 2.9 nM for the α4β2 receptors and >30 nM for the α3β2 and α3β4 receptors. In vitro autoradiography studies also indicated selective binding of [^18^F]nifrolidine to anteroventral thalamic (AVT) nucleus > thalamus > subiculum > striatum > frontal cortex > cerebellum, consistent with α4β2 receptor distribution. Nicotine (10 μM) blocked [^18^F]nifrolidine-specific binding across the brain regions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolidine%20and%20rodentia)]

Chattopadhyay et al. (6) performed biodistribution studies in rats after injection of 3.7 MBq (100 μCi) [^18^F]nifrolidine (~10 ng). A peak uptake of 0.37% injected dose (ID)/g was reached in the thalamus at 60 min, followed by a gradual washout to 0.14% ID/g at 120 min. The thalamus/cerebellum ratio at 60 min was approximately 3. The cortex (0.25% ID/g) had a higher accumulation at 60 min than the cerebellum (0.12% ID/g). Nicotine pretreatment (10 mg/kg, 5 min before tracer injection) decreased the thalamus/cerebellum ratio at 60 min to 1.8.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolidine%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolidine%20and%20%28primate%20not%20human%29)]

Chattopadhyay et al. performed a biodistribution PET study in one anesthetized male rhesus monkey injected with 155 MBq (4.2 mCi) [^18^F]nifrolidine (6) Their study showed accumulation of radioactivity in various regions of the brain, with the highest uptake in the regions of the AVT and thalamus, followed by lateral geniculate, cingulate gyrus, temporal cortex, and insular cortex. The monkey striatum and cerebellum showed lower binding than the other brain regions. The thalamus/cerebellum ratio peaked at 120 min after injection at a value of 1.7, whereas the cortex/cerebellum ratio was 1.3. [^18^F]Nifrolidine exhibited faster binding kinetics than 2-[^18^F]FA, reaching a transient equilibrium within 2.5 h.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolidine%20and%20human)]

No publication is currently available.

## NIH Support

DA 13332

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Ding Y.S., Fowler J.S., Logan J., Wang G.J., Telang F., Garza V., Biegon A., Pareto D., Rooney W., Shea C., Alexoff D., Volkow N.D., Vocci F. (2004). 6-[18F]Fluoro-A-85380, a new PET tracer for the nicotinic acetylcholine receptor: studies in the human brain and in vivo demonstration of specific binding in white matter. Synapse.
5 Kimes A.S., Horti A.G., London E.D., Chefer S.I., Contoreggi C., Ernst M., Friello P., Koren A.O., Kurian V., Matochik J.A., Pavlova O., Vaupel D.B., Mukhin A.G. (2003). 2-[18F]F-A-85380: PET imaging of brain nicotinic acetylcholine receptors and whole body distribution in humans. Faseb J.
6 Chattopadhyay S., Xue B., Collins D., Pichika R., Bagnera R., Leslie F.M., Christian B.T., Shi B., Narayanan T.K., Potkin S.G., Mukherjee J. (2005). Synthesis and evaluation of nicotine alpha4beta2 receptor radioligand, 5-(3'-18F-fluoropropyl)-3-(2-(S)-pyrrolidinylmethoxy)pyridine, in rodents and PET in nonhuman primate. J Nucl Med.
7 Pichika R., Easwaramoorthy B., Collins D., Christian B.T., Shi B., Narayanan T.K., Potkin S.G., Mukherjee J. (2006). Nicotinic alpha4beta2 receptor imaging agents: part II. Synthesis and biological evaluation of 2-[18F]fluoro-3-[2-((S)-3-pyrrolinyl)methoxy]pyridine (18F-nifene) in rodents and imaging by PET in nonhuman primate. Nucl Med Biol.